# ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-para-aminobenzoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-para-aminobenzoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ | [image]
Abbreviated name: | ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ | [image]
Synonym: | ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ | [image]
Agent Category: | Peptides | [image]
Target: | Gastrin-releasing peptide receptors (GRPR) | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^64^Cu | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of Cu-NO2A-(AMBA)-BBN(7-14)NH_2_ by Lane et al (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging)]

^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid (NO2A)-para-aminobenzoic acid (AMBA)-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (BBN(7–14)NH_2_), abbreviated as ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_, is a bombesin (BBN)-based, ^64^Cu-NO2A-conjugated peptide that was synthesized by Lane et al. for use in positron emission tomography (PET) of tumors expressing gastrin-releasing peptide receptor (GRPR) (1, 2).

GRPR is a glycosylated G-protein–coupled receptor that is normally expressed in non-neuroendocrine tissues of the breast and pancreas and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (3, 4). GRPR has been found to be overexpressed in various human tumors, and a large number of BBN analogs have been investigated for GRPR-targeted imaging and therapy (5, 6). These analogs have been synthesized on the basis of either truncated BBN ((BBN(6–14) or BBN(7–14)) or full-length BBN(1–14) (7, 8). Chelators and spacers have been used frequently for chelating metals and for improving the kinetics of conjugates (9-11).

^64^Cu is a radiometal with potential applications in diagnostic and therapeutic nuclear medicine. The half-life for ^64^Cu (t_1/2_ = 12.7 h) is long enough for drug preparation, quality control, imaging, and therapy (12, 13). However, use of ^64^Cu is limited by issues of in vivo transchelation to proteins found in blood and liver (such as superoxide dismutase) (1). A variety of chelators have been investigated for the purpose of stably chelating ^64^Cu (13). In general, ^64^Cu-labeled 1,4,7,10-tetraazacyclodecane-1,4,7,10-tetraacetic acid (^64^Cu-DOTA) and ^64^Cu-labeled 1,4,8,11-tetraazacyclotetradecane-1,4,8,11-tetraacetic acid (^64^Cu-TETA) exhibit high uptake and retention in nontarget organs, which limits their application. Cross-bridged (CB) analogs, such as CB-DO2A ((1,4,7,10-tetraazabicyclo[5.5.2]tetradecane-4,10-diyl)diacetic acid), CB-TE2A ((1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-4,11-diyl)diacetic acid), SarAr (1-N-(4-aminobenzyl)-3,6,10,13,16,19-hexa-aza-bicyclo-[6.6.6]eichosane-1,8-diamine), and NOTA (1,4,7-triazacyclononane-1,4,7-triacetic acid), demonstrate improved copper containment by enhancing the ligand's rigidity (2, 14).

Prasanphanich et al. recently reported that the NOTA-based ^64^Cu-NOTA-8-Aoc-BBN(7–14)NH_2_ (http://www.ncbi.nlm.nih.gov/books/NBK23504/) conjugate (where 8-Aoc = 8-aminooctanoic acid) exhibited decreased accumulation in hepatic tissue as compared with other chelator-based (DOTA, TETA and CB-TE2A) conjugates (2, 14). To improve the tumor uptake and maintain the good pharmacokinetic properties of the ^64^Cu-NOTA-8-Aoc-BBN(7–14)NH_2_ conjugate, Lane et al. synthesized a new group of conjugates with the NOTA derivative NO2A and replaced the spacer 8-Aoc with an aliphatic or aromatic linking (1). These conjugates were abbreviated as ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_, where X denotes the pharmacokinetic modifier, such as AMBA, β-Ala (beta-alanine), 5-Ava (5-aminovaleric acid), 6-Ahx (6-aminohexanoic acid), 8-Aoc, and 9-Anc (9-aminonanoic acid). The β-Ala, 5-Ava, 6-Ahx, and 9-Anc are aliphatic pharmacokinetic modifiers, ranging from three to nine carbons in length, whereas AMBA is an aromatic pharmacokinetic modifier and is more rigid than the aliphatic modifiers. Evidence indicates that a spacing moiety, ranging from three to eight carbons in length, can assist in receptor-mediated uptake (15). Conjugates containing an aromatic linker have significantly higher uptake and retention in PC-3 tumor tissue than those containing hydrocarbon or ether linkers (15, 16). Studies by Lane et al. have shown that the spacer X in the ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates has a significant role in clearance, accumulation, and retention of the conjugates in tumor tissue (1). ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ exhibited the highest accumulation in tumor tissue and the most efficient clearance from whole-body tissues via the renal–urinary excretion pathway. PET imaging with ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ produced high-contrast images of PC-3 tumor xenografts in severe combined immunodeficient (SCID) mice (1). This chapter describes the data obtained with ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_. Detailed information for other ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates is available in MICAD (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

- Protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) information for GRPR
- Structure information of BN and analogs in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=bombesin)
- GRPR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=GRPR%20AND%20micad%5bbook%5d)
- Chapter on ^64^Cu-NO2A-8-Aoc-BBN(7–14)NH_2_ (http://www.ncbi.nlm.nih.gov/books/NBK23504/) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

Lane et al. described the synthesis of ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates in detail (1). For ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_, the peptide AMBA-BBN(7–14)NH_2_ was synthesized with traditional F-moc chemistry. Crude peptides were obtained in ~60% yield. NOTA was conjugated to the peptide via an active ester to produce the NOTA derivative conjugate, NO2A-(AMBA)-BBN(7–14)NH_2_, with ~80% yield after purification. The calculated and observed molecular weights were both 1,344.7 for the NO2A-(AMBA)-BBN peptide conjugate^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ was synthesized with the reaction of ^64^CuCl_2_ and peptide conjugate in the presence of ammonium acetate. The radiochemical yield was >90%. All of the unconjugated peptide precursors, peptide conjugates, and metallated peptide conjugates were purified with reverse-phase high-performance liquid chromatography (RP-HPLC) and characterized with mass spectrometry. The radiochemical purity and specific activity were not described.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

The stability of ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ in human serum albumin was determined with quantification of the ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ peak area in the radiometric RP-HPLC chromatogram. The percent of intact conjugate was >80% after 24 h incubation (37°C, 5% CO_2_-enriched atmosphere) with human serum albumin (1).

A competitive displacement binding assay was performed in PC-3 cells with ^125^I-(Tyr^4^)-BBN as the radioligand (1). High binding affinities were observed for both unlabeled NO2A-(AMBA)-BBN(7–14)NH_2_ (inhibition constant (K_i_) = 4.61 ± 1.54 nM) and ^nat^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ (^nat^Cu = natural copper) (K_i_ = 15.45 ± 2.88 nM).

Internalization was determined after incubation of the PC-3 cells with ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ for different times. Externalization was determined after an initial 40-min internalization period in PC-3 cells. The results revealed GRPR-mediated trapping of radioactivity inside the cells with very little externalization of ^64^Cu with cells washed after the internalization period (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

Biodistribution studies of ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ were performed in both normal CF-1 mice (n = 4 or 5/group) and PC-3 xenograft-bearing SCID mice (n = 5 mice/group per time point). The biodistribution data were compared among the ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates (where X = β-Ala, 5-Ava, 6-Ahx, 8-Aoc, 9-Anc, or AMBA) (1, 2).

In normal mice, rapid clearance from blood was observed for all conjugates, with ≤0.5% injected dose per gram tissue (% ID/g) remaining in circulation at 1 h after injection (for ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_, 0.28 ± 0.05% ID/g). Excretion properties of the conjugates were directly related to the length of X. Increasing the hydrophobicity of the conjugate (increasing the aliphatic length of X) led to higher excretion rates via the hepatobiliary system. The more hydrophilic conjugate, ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_, had a lesser degree of accumulation in hepatic tissue (0.70 ± 0.08% ID/g at 1 h after injection). Uptake of the conjugates in GRPR-expressing pancreas ranged from 15.10 to 30.63% ID/g at 1 h after injection with 30.63 ± 3.26% ID/g for ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_, indicating effective GRPR targeting for the radiolabeled conjugates. The four conjugates showing the most favorable pharmacokinetic properties and the highest degree of pancreas accumulation were those in which X = 6-Ahx, 8-Aoc, 9-Anc, or AMBA, which were further studied in PC-3 tumor-bearing SCID mice (1).

In tumor-bearing SCID mice, all four conjugates were cleared effectively from the bloodstream, with 0.93–1.35% ID/g remaining at 1 h after injection (for ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_, 1.35 ± 0.51% ID/g). Excretion routes were similar to those observed in normal CF-1 mice, with more hydrophobic conjugates excreted through the hepatobiliary system. Minimal accumulation of radioactivity was observed in the liver at 24 h, ranging from 0.68 to 1.37% ID/g (for ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_, 1.23 ± 0.25% ID/g), suggesting that the metal complex was effectively stable under in vivo conditions. High receptor-mediated accumulation was observed in both the pancreas and tumor for all conjugates. Tumor uptake of the ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ was 6.05 ± 1.15, 3.66 ± 0.54, and 2.54 ± 0.48% ID/g at 1 h, 4 h, and 24 h after injection, respectively. Pancreas uptake of the ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ was 37.34 ± 4.83, 22.50 ± 3.13, and 8.93 ± 1.81% ID/g at 1 h, 4 h, and 24 h after injection, respectively. When comparing the tumor/tissue ratios at 24 h after injection, ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ showed optimal tumor/blood, tumor/kidney, and tumor/liver ratios, with values of 2.6, 2.8, and 2.1, respectively (1).

PET imaging was performed at 18 h after tail-vein injection of ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ (where X = 6-Ahx, 8-Aoc, 9-Anc, or AMBA) (1). The PC-3 tumors were clearly identifiable in PET images for all conjugates. Tumor/background ratios decreased with increased length of X, which appears to be a function of increasing the hydrophobicity of the conjugate. ^64^Cu-NO2A-(AMBA)-BBN(7–14)NH_2_ demonstrated superior tumor targeting and retention, with clear tumor contrast from surrounding tissue and minimal abdominal accumulation. In comparison, for ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = 6-Ahx, high tumor uptake with relatively high kidney accumulation was observed. For ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = 8-Aoc, high tumor and liver uptake values were observed. For ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = 9-Anc, moderate tumor uptake with significant abdominal accumulation (liver and gastrointestinal tract) was observed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Lane S.R., Nanda P., Rold T.L., Sieckman G.L., Figueroa S.D., Hoffman T.J., Jurisson S.S., Smith C.J. (2010). Optimization, biological evaluation and microPET imaging of copper-64-labeled bombesin agonists, [64Cu-NO2A-(X)-BBN(7-14)NH2], in a prostate tumor xenografted mouse model. Nucl Med Biol.
2 Prasanphanich A.F., Retzloff L., Lane S.R., Nanda P.K., Sieckman G.L., Rold T.L., Ma L., Figueroa S.D., Sublett S.V., Hoffman T.J., Smith C.J. (2009). In vitro and in vivo analysis of [(64)Cu-NO2A-8-Aoc-BBN(7-14)NH(2)]: a site-directed radiopharmaceutical for positron-emission tomography imaging of T-47D human breast cancer tumors. Nucl Med Biol.
3 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
4 Erspamer V., Erpamer G.F., Inselvini M. (1970). Some pharmacological actions of alytesin and bombesin. J Pharm Pharmacol.
5 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
6 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
7 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
8 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
9 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
10 Mu L., Honer M., Becaud J., Martic M., Schubiger P.A., Ametamey S.M., Stellfeld T., Graham K., Borkowski S., Lehmann L., Dinkelborg L., Srinivasan A. (2010). In vitro and in vivo characterization of novel 18F-labeled bombesin analogues for targeting GRPR-positive tumors. Bioconjug Chem.
11 Becaud J., Mu L., Karramkam M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Lehmann L., Borkowski S., Berndorff D., Dinkelborg L., Srinivasan A., Smits R., Koksch B. (2009). Direct one-step 18F-labeling of peptides via nucleophilic aromatic substitution. Bioconjug Chem.
12 Wadas T.J., Wong E.H., Weisman G.R., Anderson C.J. (2007). Copper chelation chemistry and its role in copper radiopharmaceuticals. Curr Pharm Des.
13 Hoffman T.J., Smith C.J. (2009). True radiotracers: Cu-64 targeting vectors based upon bombesin peptide. Nucl Med Biol.
14 Prasanphanich A.F., Nanda P.K., Rold T.L., Ma L., Lewis M.R., Garrison J.C., Hoffman T.J., Sieckman G.L., Figueroa S.D., Smith C.J. (2007). [64Cu-NOTA-8-Aoc-BBN(7-14)NH2] targeting vector for positron-emission tomography imaging of gastrin-releasing peptide receptor-expressing tissues. Proc Natl Acad Sci U S A.
15 Smith C.J., Gali H., Sieckman G.L., Higginbotham C., Volkert W.A., Hoffman T.J. (2003). Radiochemical investigations of (99m)Tc-N(3)S-X-BBN[7-14]NH(2): an in vitro/in vivo structure-activity relationship study where X = 0-, 3-, 5-, 8-, and 11-carbon tethering moieties. Bioconjug Chem.
16 Garrison J.C., Rold T.L., Sieckman G.L., Naz F., Sublett S.V., Figueroa S.D., Volkert W.A., Hoffman T.J. (2008). Evaluation of the pharmacokinetic effects of various linking group using the 111In-DOTA-X-BBN(7-14)NH2 structural paradigm in a prostate cancer model. Bioconjug Chem.